# 1,1’-bis-(4-sulfobutyl)indotricarbocyanine-5,5’-dicarboxylic acid diglucamide monosodium salt

Chemical name: | 1,1'-bis-(4-sulfobutyl)indotricarbocyanine-5,5'-dicarboxylic acid diglucamide monosodium salt
Abbreviated name: | SIDAG
Synonym:
Agent Category: | Peptide
Target: | Non-targeted
Target Category: | Binding
Method of detection: | Optical imaging (NIRF)
Source of signal: | SIDAG
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20AND%20dye)]http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed

In recent years, an increasing number of imaging studies have been carried out using all-optical, imaging technology that absorb and emit in the near-infrared (NIR) spectrum (1-4). NIR imaging has the advantage of reducing the background and scattering through biological tissue usually encountered with fluorescent imaging in live animals with short wavelengths of light.

The indocyanine green (ICG) is a well-known, clinically approved, carbocyanine non-specific NIR-fluorescent dye (5, 6) used for example for testing hepatic functions (7). It has been investigated as a potential contrast agent in animals (8) and in humans for the detection of breast tumors (9). ICG presents major disadvantages that make its use very limited: a high level of plasma protein binding (up to 98% a few seconds after injection), a rapid clearance by the liver, a low stability in aqueous media and a poor fluorescence efficiency (5, 10).

Major effort is being made in designing new NIR-absorbing and fluorescing probes with more favorable characteristics, such as a high hydrophilicity and low levels of plasma protein binding. One of them, 1,1'-bis-(4-sulfobutyl)indotricarbocyanine-5,5'-dicarboxylic acid diglucamide monosodium salt (SIDAG), is a highly hydrophilic derivative based on a carbocyanine chromophore identical to ICG, and showing a low plasma binding of ~10%.

SIDAG It has an estimated blood half-life of ~200 min, is 60 times more biocompatible than ICG (5), less toxic (11), and has a significantly greater fluorescent yield compared with ICG (5, 12). Its absorption and emission maximum wavelengths are 800 and 830 nm respectively.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20AND%20dye)]http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed

Synthesis details for preparing SIDAG were reported by Licha et al. (5) in 2000. The procedure described by the authors involved a derivatization of the symmetric dicarboxylated indotricarbocyanine bis-1,1'-(4-sulfobutyl)indotricarbocyanine-5,5'-dicarboxylic with the amino-sugar D-glucamine, leading to the final symmetric diglucamide SIDAG (0.75g, 53% yield). After purification by chromatography, SIDAG was obtained as a salt. The indotricarbocyanine was obtained in 77% yield by reaction of the carboxylated indolenine, 5-carboxy-1-(4-sulfobutyl)-2,3,3,-trimethyl-3H-indolenine with 1-(4-sulfobutyl)-2,3,3-trimethyl-3H-indolenine, both synthesized following the procedures previously described in the literature (13, 14). Details on the various intermediary steps involved in the synthesis of SIDAG can be found in (5).

The partition coefficient (n-butanol/water) reported by Licha et al. (5) was <0.005 and the equilibrium plasma protein binding was ~ 10% (maximum standard deviation of 10% of value, 3 measurements performed). Measurements of the absorption maxima λ_max,abs_ (nm), fluorescence emission maxima λ_max,em_ (nm), molar absorption coefficients є (l.mol^-1^.cm^-1^) and fluorescence quantum yields Ф (based on ICG as standard, Ф_ICG_ = 0.13) were also made by the authors and the following respective values were obtained: 753, 790, 201 000, 0.066 with PBS as solvent, and 755, 70, 252 000, 0.076 in plasma.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20dye%20AND%20in%20vitro)]

A value of ~10% plasma protein binding for SIDAG (obtained by equilibrium dialysis) was reported in the literature by Paumgarten et al. (15) in 1970. Other measurements performed by ultrafiltration using 400µl of a 0.5mg/ml solution of SIDAG in spiked mouse serum were reported in details by Perlitz et al. (16) in 2005. The experimental protocol followed by Perlitz et al. involved incubating the dye solution at 37°C for 1h, centrifuging it for 8 min at 1500g, and subsequently performing absorbance and emission measurements with an excitation wavelength of 700nm. The resulting quantum yield obtained for SIDAG was 6.5% (with the quantum yield from ICG in DMSO (Ф_ICG_ = 0.13) used as standard (9)), and the measured free fraction was 40%. Those values appeared to be in agreement with the previous results reported by Paumgarten et al. (15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20AND%20rodentia%5BMeSH%5D)]

Perlitz et al. (16) investigated the ability of SIDAG to be used as a contrast agent in in vivo imaging of subcutaneously grown tumors, using F9-teratocarcinoma bearing mice (n=8, tumor volumes = 100 to 950 mm^3^, manganese-free diet to reduce auto-fluorescence). The experimental protocol involved injecting intravenously a physiological saline solution of dye (2 µmol/kg of body) into the tail vein, and recording fluorescence signals at 1, 10, 30 min and 1, 4, 7, 24 and 48 h after injection. Tumor tissue and non-diseased tissue (control region) were selected as regions of interest (ROIs). Quantification of the fluorescence intensities in the ROIs were made using a special NIR-XP software, as detailed in the article (16).

A maximum of fluorescence intensity of approximately a million counts was reached at 10 min after injection (versus 1,100,000 counts in the control regions at that same time). After 4 h, the fluorescence intensity was below 100,000 counts, with higher values in the tumor than in the control region. A discrimination of the tumor from its surrounding areas was observed 4 h after injection, and was still clearly visible for 48 h. A strong fluorescence from kidneys was recorded at 4 and 7 h post-injection, suggesting renal uptake. Because differences in fluorescence intensities between tumor and control regions remained constant for the all 48 h, Perlitz et al. (16) suggested that a tubular re-absorption of a certain amount of dye was re-entering the circulation and leading to prolonged contrasts between tumor and control tissue. Using a two-compartment model, the authors estimated the renal elimination half-life to be 220 min.

Fischer et al. (11) performed NIRF studies using ICG- and SIDAG-NIRF to determine whether normal and inflammatory joints can be differentiated through kinetic properties of those non-specific dyes. The experimental setup involved using 20 healthy mice and 20 mice with induced Lyme arthritis (n=10 for ICG, n=10 for SIDAG for both healthy and arthritic groups). Each group of mice injected with either dye was divided into two sub-groups (n=5): sub-group 1 one received the dye at 1.0µmol/kg of tissue, and sub-group 2 was injected with a solution at 2.0µmol/kg. Data were acquired from ankle joints of the mice, using short exposure times (0.2 s).

Results showed that such technique was indeed able to detect early stages of arthritis, and that SIDAG was retained more readily in inflamed tissues than ICG, providing a sufficient spatial resolution even for small structures within the joints. After injection of SIDAG, a slow increase in fluorescence signal was observed throughout the 150 min observation period, with AUCs of 220 ± 60 counts (sub-group 1) and 290 ± 90 counts (sub-group 2). Histological examination showed a difference of histological score between control and arthritis groups of ~3 (1.7 ± 1.7 versus 6.2 ± 3.2; P < 0.05). The detection of inflammation in the joints was found possible at 24h post-injection with SIDAG, but not with ICG. Nevertheless, several limitations were noted by the authors, including the fact that the interval of image acquisition after bolus injection had to be very short, explaining why the peak enhancement after SIDAG was missed.

Licha et al. (5) investigated the efflux behavior of SIDAG as a function of its physicochemical properties, both for healthy and tumor tissues in 9L-glioma-bearing Fischer rats (animal weight = 290 to 350g, tumor volume = ~5 ml). SIDAG was intravenously injected at a concentration of 0.5 µmol/kg of body weight, 2 min after signal recording. A slow clearance of the dye was observed, with calculated half-life times of 75 min for the tumor and 115 min for the control site (assuming a mono-exponential decay). The authors reported a maximal contrast of 1.78 reached at 7 min post-injection, with a subsequent decrease to the native level of 1.3 at ~100 min post-injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20dye%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20dye%20AND%20%28primates%20NOT%20human%20OR%20baboon%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SIDAG%20dye%20AND%20human)]

No publication is currently available.

## References

1 Nesterov EE, Skoch J, Hyman BT, Klunk WE, Bacskai BJ, Swager TM. (2005). In vivo optical imaging of amyloid aggregates in brain: design of fluorescent markers. Angew Chem Int Ed Engl.
2 Skoch J, Dunn A, Hyman BT, Bacskai BJ. (2005). Development of an optical approach for noninvasive imaging of Alzheimer's disease pathology. J Biomed Opt.
3 Frangioni JV. (2006). Self-illuminating quantum dots light the way. Nat Biotechnol.
4 Hintersteiner M, Enz A, Frey P, Jaton AL, Kinzy W, Kneuer R, Neumann U, Rudin M, Staufenbiel M, Stoeckli M, Wiederhold KH, Gremlich HU. (2005). In vivo detection of amyloid-beta deposits by near-infrared imaging using an oxazine-derivative probe. Nat Biotechnol.
5 Licha K, Riefke B, Ntziachristos V, Becker A, Chance B, Semmler W. (2000). Hydrophilic cyanine dyes as contrast agents for near-infrared tumor imaging: synthesis, photophysical properties and spectroscopic in vivo characterization. Photochem Photobiol.
6 Ebert B, Sukowski U, Grosenick D, Wabnitz H, Moesta KT, Licha K, Becker A, Semmler W, Schlag PM, Rinneberg H. (2001). Near-infrared fluorescent dyes for enhanced contrast in optical mammography: phantom experiments. J Biomed Opt.
7 Caesar J, Shaldon S, Chiandussi L, Guevara L, Sherlock S. (1961). The use of indocyanine green in the measurement of hepatic blood flow and as a test of hepatic function. Clin Sci.
8 Reynolds JS, Troy TL, Mayer RH, Thompson AB, Waters DJ, Cornell KK, Snyder PW, Sevick-Muraca EM. (1999). Imaging of spontaneous canine mammary tumors using fluorescent contrast agents. Photochem Photobiol.
9 Ntziachristos V, Yodh AG, Schnall M, Chance B. (2000). Concurrent MRI and diffuse optical tomography of breast after indocyanine green enhancement. Proc Natl Acad Sci U S A.
10 Landsman ML, Kwant G, Mook GA, Zijlstra WG. (1976). Light-absorbing properties, stability, and spectral stabilization of indocyanine green. J Appl Physiol.
11 Fischer T, Gemeinhardt I, Wagner S, Stieglitz DV, Schnorr J, Hermann KG, Ebert B, Petzelt D, Macdonald R, Licha K, Schirner M, Krenn V, Kamradt T, Taupitz M. (2006). Assessment of unspecific near-infrared dyes in laser-induced fluorescence imaging of experimental arthritis. Acad Radiol.
12 Riefke B, Licha K, Semmler W. (1997). Radiologe.
13 Terpetschnig E, Szmacinski H, Ozinskas A, Lakowicz JR. (1994). Synthesis of squaraine-N-hydroxysuccinimide esters and their biological application as long-wavelength fluorescent labels. Anal Biochem.
14 Mujumdar RB, Ernst LA, Mujumdar SR, Waggoner AS. (1989). Cyanine dye labeling reagents containing isothiocyanate groups. Cytometry.
15 Paumgarten G, Probst P, Kraines K, Leevy CM. (1970). Kinetics of indocyanine green removal from the blood. N.Y. Acad. Sci.
16 Perlitz C, Licha K, Scholle FD, Ebert B, Bahner M, Hauff P, Moesta KT, Schirner M. (2005). Comparison of two tricarbocyanine-based dyes for fluorescence optical imaging. J Fluoresc.